# ^111^In-Benzyl-diethylenetriamine pentaacetic acid-AMB8LK

Chemical name: | ^111^In-Benzyl-diethylenetriamine pentaacetic acid-AMB8LK
Abbreviated name: | ^111^In-Bz-DTPA-AMB8LK, ^111^In-DTPA-AMB8LK
Synonym:
Agent Category: | Antibody
Target: | Ferritin
Target Category: | Antibody binding
Method of detection: | SPECT, gamma planar
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=306744), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=91718887) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2512) for more information about ferritin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AMB8LK)]

Ferritin is an iron storage protein with a molecular mass of 440 kDa and is overexpressed in some tumors such as breast cancer (1, 2), Hodgkin's lymphoma (3), and pancreatic cancer (4, 5). Iron has the ability to promote neoplastic cell growth (6). Radiolabeled polyclonal anti-ferritin antibodies have been shown to have anti-tumor effects in patients with Hodgkin’s lymphoma. However, the response rate was dependent on the batches of polyclonal antibody used. Therefore, AMB8LK, a murine IgG_1_ monoclonal antibody (mAb) against ferritin extracted from human spleen with an affinity constant (K_d_) of 5.1 nM, was conjugated with ^111^In via the bifunctional linker benzyl-diethylenetriamine pentaacetic acid (Bz-DTPA). ^111^In-DTPA-AMB8LK is being evaluated for imaging of pancreatic cancer (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AMB8LK%20and%20synthesis)]

AMB8LK mAb was conjugated to 2-(4-isothiocyanatobenzyl)-diethylenetriamine pentaacetic acid (PSCN-Bz-DTPA) at 37°C overnight (7). Bz-DTPA-AMB8LK was purified by ultrafiltration. There are ~2 DTPA per mAb. BZ-DTPA-AMB8LK (0.05 mg) was mixed with 6.5 MBq (0.18 mCi) of ^111^InCl_3_ .The mixture was incubated for 30 min at room temperature. The labeling efficiency was ~95% of ^111^In incorporation. Specific activities of the preparations were >6 GBq/μmol (0.16 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AMB8LK%20and%20in%20vitro)]

In vitro binding tests showed that immunoreactivity to ferritin of ^111^In-DTPA-AMB8LK was ~87% (7). The immunoreactivity to ferritin on human pancreatic ductal adenocarcinoma CAPAN-1 cells (fixed and permeabilized) was ~52%. ^111^In-DTPA-AMB8LK lost <3% of activity in plasma at 37°C for 7 days.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AMB8LK%20and%20rodentia)]

Sabbah et al. (7) monitored biodistribution after injection of 0.2 MBq (5.4 μCi) ^111^In-DTPA-AMB8LK in normal nude mice (n = 4/group). Of all organs, the liver showed the highest ^111^In-DTPA-AMB8LK uptake of 7.0% injected dose/g (ID/g) at 24 h, 7.1% at 48 h, and 7.5% at 72 h. Other organs that showed significant levels of uptake were the bones (1.7–2.1% ID/g) and intestine (2.9–3.2% ID/g). Uptake in the muscle, lung, and kidneys was <2%, and uptake in the stomach and spleen was <1%. Radioactivity in the blood was 15.8% ID/g at 24 hr and 12.6% ID/g at 72 h. In a second series of experiments, biodistribution of ^111^In- DTPA-AMB8LK via injection (0.2 MBq (5.4 μCi)) was studied in nude mice (n = 4/group) bearing human pancreatic ductal adenocarcinoma CAPAN-1 xenografts at 24, 48, and 72 h. In addition to the organs analyzed during the experiments in normal mice, radioactivity levels in the tumor and pancreas were measured. Tumor uptake of ^111^In-DTPA-AMB8LK was 12.8% ID/g at 24 h and 23.6% at 72 h. The accumulation of radioactivity in the pancreas was <0.2% ID/g at all time points. Uptake in other organs was similar in the normal mice. Single-photon emission computed tomography imaging of a mouse bearing a CAPAN-1 tumor revealed that the majority of radioactivity was in the urinary bladder and heart, followed by the liver and lung at 1 h. The tumor was clearly visualized at 24 h with some ^111^In- DTPA-AMB8LK still visualized in the heart and liver. Radioactivity was still present at 72 h in the tumor but not in the heart and liver. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AMB8LK%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AMB8LK%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AMB8LK%20and%20human)]

No publication is currently available.

## References

1 Guner G., Kirkali G., Yenisey C., Tore I.R. (1992). Cytosol and serum ferritin in breast carcinoma. Cancer Lett.
2 Weinstein R.E., Bond B.H., Silberberg B.K., Vaughn C.B., Subbaiah P., Pieper D.R. (1989). Tissue ferritin concentration and prognosis in carcinoma of the breast. Breast Cancer Res Treat.
3 Eshhar Z., Order S.E., Katz D.H. (1974). Ferritin, a Hodgkin's disease associated antigen. Proc Natl Acad Sci U S A.
4 Drysdale J.W., Adelman T.G., Arosio P., Casareale D., Fitzpatrick P., Harzard J.T., Yokota M. (1977). Human isoferritins in normal and disease states. Semin Hematol.
5 Marcus D.M., Zinberg N. (1974). Isolation of ferritin from human mammary and pancreatic carcinomas by means of antibody immunoadsorbents. Arch Biochem Biophys.
6 Weinberg E.D. (1996). The role of iron in cancer. Eur J Cancer Prev.
7 Sabbah E.N., Kadouche J., Ellison D., Finucane C., Decaudin D., Mather S.J. (2007). In vitro and in vivo comparison of DTPA- and DOTA-conjugated antiferritin monoclonal antibody for imaging and therapy of pancreatic cancer. Nucl Med Biol.